# Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_
Abbreviated name: | Gd-DOTA-cFlFlFK, Gd.1
Synonym:
Agent category: | Peptide
Target: | Formyl peptide receptor type 1 (FPR1)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images. Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (2, 3).

The formyl peptide receptor (FPR) family consists of three receptor subtypes (FPR1–FPR3) (4). These G-protein–coupled receptors are found on leukocytes. FPR1 is highly expressed on neutrophils under inflammatory conditions for their emigration to the sites of injury and infection (5). However, collateral damage may occur, which can cause pain, edema, fever, and swelling. The peptide antagonist cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_ (cFlFlFK) specifically binds FPR1 on neutrophils (6). The peptide was conjugated with Gd-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid to the ε-amino group of Lys to form Gd-DOTA-cFlFlFK for use with MRI imaging of neutrophils at the sites of inflammation (7).

### Related Resource Links:

- Chapters in MICAD (cFlFlFK (http://www.ncbi.nlm.nih.gov/books/?term=cFlFlFK+AND+micad%5Bbook%5D))
- Gene information in NCBI (FPR1 (http://www.ncbi.nlm.nih.gov/gene/2357))
- Articles in Online Mendelian Inheritance in Man (OMIM) (FPR1 (http://www.ncbi.nlm.nih.gov/omim/136537))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+synthesis)]

The DOTA motif was conjugated to the ε-amino group of Lys in cFlFlFK (1.3 µmol) using DOTA-N-hydroxysuccinimide (1.3 µmol) in sodium borate buffer for 12 h at 4°C (7). DOTA-cFlFlFK (one DOTA moiety per conjugate) was purified with high-performance liquid chromatography with 65% yield, and its molecular weight was confirmed with mass spectroscopy. DOTA-cFlFlFK (1 µmol) was incubated with GdCl_3_ (1 µmol) for 3 h at room temperature in water (pH 5.5). Gd-DOTA-cFlFlFK was purified with column chromatography with 88% yield, and its molecular weight was confirmed with mass spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+in+vitro)]

Gd-DOTA-cFlFlFK exhibited an r_1_ relaxivity value of 5.4 mM^–1^s^–1^ (9.4 T) (7). Gd-DOTA exhibited an r_1_ relaxivity value of 4.2 mM^–1^s^–1^. In vitro receptor-binding assays were performed using human embryonic kidney cells stably expressing FPFR1 and ^125^I-fMLP analog as the radioligand. Gd-DOTA-cFlFlFK and cFlFlFK exhibited affinity binding constant (K_d_) values of 4.5 nM and 2.0 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+rodentia)]

Stasiuk et al. (7) performed dynamic T1-weighted MRI (9.4 T) studies with intravenous injection of 1 mmol Gd/kg Gd-DOTA-cFlFlFK or Gd-DOTA in mice (number of mice was not reported) pretreated with lipopolysaccharide (intraperitoneally, 24 h) to cause sites of inflammation by disrupting the vascular endothelium. There was a marked increase in signal intensity around the right ear at 8 min after injection of Gd-DOTA-cFlFlFK. The signal intensity continued to increase over a 20-min period and then leveled off and remained stable for 80 min. On the other hand, no such increase in signal intensity was observed with Gd-DOTA for 80 min. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
3 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
4 Ye R.D., Boulay F., Wang J.M., Dahlgren C., Gerard C., Parmentier M., Serhan C.N., Murphy P.M. (2009). International Union of Basic and Clinical Pharmacology. LXXIII. Nomenclature for the formyl peptide receptor (FPR) family. Pharmacol Rev.
5 Loitto V.M., Rasmusson B., Magnusson K.E. (2001). Assessment of neutrophil N-formyl peptide receptors by using antibodies and fluorescent peptides. J Leukoc Biol.
6 Gavins F.N. (2010). Are formyl peptide receptors novel targets for therapeutic intervention in ischaemia-reperfusion injury?. Trends Pharmacol Sci.
7 Stasiuk G.J., Smith H., Wylezinska-Arridge M., Tremoleda J.L., Trigg W., Luthra S.K., Morisson Iveson V., Gavins F.N., Long N.J. (2013). Gd3+ cFLFLFK conjugate for MRI: a targeted contrast agent for FPR1 in inflammation. Chem Commun (Camb).